# Hoechst 33258-polyethylene glycol-IR-786

Chemical name: | Hoechst 33258-polyethylene glycol-IR-786
Abbreviated name: | Hoechst-IR
Synonym:
Agent category: | Compound
Target: | DNA
Target category: | Nucleic acid
Method of detection: | Optical, near-infrared fluorescence (NIR) imaging
Source of signal\contrast: | IR-786
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=IR-786%5BAll%20Fields%5D)]

Optical fluorescence imaging is increasingly used to observe biological functions of specific targets (1, 2). However, the intrinsic fluorescence of biomolecules poses a problem when visible fluorophores that absorb light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–900 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a noninvasive alternative to radionuclide imaging in small animals or with probes in close proximity of the target in humans. Among the various optical imaging agents, only indocyanine green (ICG (http://dailymed.nlm.nih.gov/dailymed/drugInfo.cfm?id=15096)), with NIR fluorescence absorption at 780 nm and emission at 820 nm, is approved by the United States Food and Drug Administration for clinical applications in angiography, blood flow evaluation, and liver function assessment. It is also under evaluation in several clinical trials (http://clinicaltrials.gov/ct2/results?term=indocyanine+green) for other applications, such as optical imaging and mapping of both the lymphatic vessels and lymph nodes in cancer patients for surgical dissection of tumors and endoscopic imaging of the pancreas and colon.

Necrosis is a central characteristic in the pathophysiology of many diseases, such as cancer, neurodegenerative disorders, cardiovascular disorders, atherosclerosis, and sepsis (3, 4). During cell necrosis, the cellular contents, including genomic DNA, are released into extracellular space (5, 6). The extracellular DNA (E-DNA) is high in the extracellular space in tissues with high levels of necrosis. On the other hand, E-DNA is not generated during apoptosis (programmed cell death) of healthy cells; therefore, the E-DNA content in healthy tissues should be low. Hoechst 33258 is a fluorescence dye (excitation, 350 nm) that binds DNA with high affinity (K_d_ = 1–3 nM) (7). IR-786 is a heptamethine indocyanine-type NIR fluorophore with peak absorption of 760–780 nm and peak excitation emission of 795–815 nm (8). IR-786 provides a quantum yield of 3.3%. Dasari et al. (9) linked Hoechst 33258 and IR-786 with an 11-unit polyethylene glycol (PEG) linker to form Hoechst-PEG-IR-786 (Hoechst-IR). Unlike Hoechst 33258, Hoechst-IR does not cross the cell membrane of healthy cells to bind intracellular DNA. Hoechst-IR has been evaluated for in vivo NIR imaging of E-DNA released from necrotic tissue in a myocardial infarction model and lipopolysaccharide/D-galactosamine (LPS/GaIN)-induced sepsis.

### Related Resource Links:

- Chapters in MICAD (IR-786 (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=IR-786+AND+micad%5Bbook%5D), nucleic acid (http://www.ncbi.nlm.nih.gov/books/?term=siRNA+OR+nucleic+acid+OR+oligonucleotide+AND+micad%5Bbook%5D+AND+table%5Btype%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=IR-786%5BAll%20Fields%5D%20AND%20%28%22chemical%20synthesis%22%5BSubheading%5D%20OR%20synthesis%5BAll%20Fields%5D%29)]

Hoechst-IR was prepared by conjugation of Hoechst amine PEG_3_ derivative with IR-786 PEG_8_ derivative active ester with 31% yield (9). The structure of Hoechst-IR was confirmed with nuclear magnetic resonance spectroscopy and mass spectroscopy.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=IR-786%5BAll%20Fields%5D%20AND%20in%20vitro)]

Dasari et al. (9) performed saturation-binding studies of Hoechst-IR with a 22-base-pair double-stranded oligonucleotide. Hoechst-IR exhibited a K_d_ value of 0.21 nM. Cellular uptake of Hoechst-IR was performed with 30 min incubation with RAW 264.7 macrophages or methanol-fixed macrophages. Fluorescence microscopy showed that low levels of intracellular signal were detected in the live cells because Hoechst-IR does not permeate the cell membrane efficiently. In contrast, high levels of intracellular signal were observed in the methanol-treated cells. In addition, Hoechst 33258 crossed the cell membrane of the live cells and bound to intracellular DNA.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=IR-786%5BAll%20Fields%5D%20AND%20rodentia)]

Dasari et al. (9) performed ex vivo imaging with Hoechst-IR in a myocardial ischemia reperfusion injury mouse model. The left anterior descending coronary artery was ligated for 30 min with subsequent perfusion for 2 h, followed by retro-orbital injection of 10 nmol Hoechst-IR (n = 3 mice). Three sham-operated mice were also studied with injection of Hoechst-IR. The hearts were excised at 1 h after injection for NIR imaging. Hoechst-IR accumulated one-fold higher in the necrotic zone of the infarcted myocardium than in the necrotic zone of the myocardium of sham-operated mice (P < 0.05). In another experiment, sepsis was induced in mice with an intraperitoneal injection of LPS-GaIN or saline, followed by intravenous injection of Hoechst-IR (3.5 µmol/kg) at 24 h after sepsis induction. Whole-body NIR fluorescence imaging studies of the mice (n = 5/group) were then performed at 24 h after Hoechst-IR injection. The total fluorescence intensity from the lung area was integrated. Signal intensity was three-fold higher in the lungs from the mice with sepsis than in the lungs from the mice treated with saline (P < 0.05).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=IR-786%5BAll%20Fields%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29%20)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=IR-786%5BAll%20Fields%5D%20AND%20primate%20NOT%20human)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=IR-786%5BAll%20Fields%5D%20AND%20human)]

No publication is currently available.

## NIH Support

U01 HL80711-01, R01 HL80711-01

## References

1 Gurfinkel M., Ke S., Wen X., Li C., Sevick-Muraca E.M. (2003). Near-infrared fluorescence optical imaging and tomography. Dis Markers.
2 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
3 Amaravadi R.K., Thompson C.B. (2007). The roles of therapy-induced autophagy and necrosis in cancer treatment. Clin Cancer Res.
4 Artal-Sanz M., Tavernarakis N. (2005). Proteolytic mechanisms in necrotic cell death and neurodegeneration. FEBS Lett.
5 Pisetsky D.S., Fairhurst A.M. (2007). The origin of extracellular DNA during the clearance of dead and dying cells. Autoimmunity.
6 Jahr S., Hentze H., Englisch S., Hardt D., Fackelmayer F.O., Hesch R.D., Knippers R. (2001). DNA fragments in the blood plasma of cancer patients: quantitations and evidence for their origin from apoptotic and necrotic cells. Cancer Res.
7 Rajur S.B., Robles J., Wiederholt K., Kuimelis R.G., McLaughlin L.W. (1997). Hoechst 33258 Tethered by a Hexa(ethylene glycol) Linker to the 5'-Termini of Oligodeoxynucleotide 15-Mers: Duplex Stabilization and Fluorescence Properties. J Org Chem.
8 Tanaka E., Choi H.S., Humblet V., Ohnishi S., Laurence R.G., Frangioni J.V. (2008). Real-time intraoperative assessment of the extrahepatic bile ducts in rats and pigs using invisible near-infrared fluorescent light. Surgery.
9 Dasari M., Lee S., Sy J., Kim D., Brown M., Davis M., Murthy N. (2010). Hoechst-IR: an imaging agent that detects necrotic tissue in vivo by binding extracellular DNA. Org Lett.